# Cd^125m^Te/ZnS Nanoparticles coupled with anti-thrombomodulin monoclonal antibody 201B

Chemical name: | Cd^125m^Te/ZnS Nanoparticles coupled with anti-thrombomodulin monoclonal antibody 201B
Abbreviated name: | Cd^125m^Te/ZnS-201B
Synonym:
Agent category: | Antibody
Target: | Lung thrombomodulin
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal\contrast: | ^125m^Te
Activation: | No
Studies: | - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/339657), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/237681095) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7056) for more information about thrombomodulin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=201B)]

Cd^125m^Te/ZnS nanoparticles consist of Cd^125m^Te cores capped with ZnS to prevent particle degradation and to reduce leaching of ^125m^Te (t_1/2_ = 58 days, x-ray = 27–30 keV, and gamma ray = 35.5 keV) into blood stream and tissues. They can be derivatized for conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies. Cd^125m^Te/ZnS nanoparticles have a diameter of ~5 nm. There have been limited in vivo studies of the toxicological and pharmacological profiles of Cd^125m^Te/ZnS in small animals (1). Thrombomodulin (CD141 or BDCA-3) is an integral membrane receptor protein expressed on the surface of endothelial cells (2). Thrombin binds to thrombomodulin to participate in coagulation, inflammation, and cancer (3). Monoclonal antibody (mAb) 201B against mouse lung thrombomodulin has been coupled to Cd^125m^Te/ZnS nanoparticles for single-photon emission computed tomography (SPECT) biodistribution studies in mice (4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cd+201B+synthesis)]

Woodward et al. (4) prepared Cd^125m^Te nanoparticles by incubation of ^125m^Te with CdO and tetradecylphosphonic acid at 250°C for 5 min. Cd^125m^Te nanoparticles were incubated with zinc diethydithiocarbamate in trioctylphosphine solution at 250°C for 2 h to form Cd^125m^Te/ZnS nanoparticles. Cd^125m^Te/ZnS nanoparticles were treated with excess mercaptoacetic acid at 60°C for 1 h. A reaction mixture containing 0.05 mM Cd^125m^Te nanoparticles, 2 nmol antibody (201B or control mAb 33), 5 mM N-hydroxysulfosuccinimide, 0.05 M 1-ethyl-3(3-dimethylaminopropyl)carbodiimide hydrochloride in phosphate-buffered saline (PBS; pH, 7.0) was incubated at room temperature for 2−4 h, then stored at 4°C overnight. Cd^125m^Te/ZnS-201B nanoparticles were purified with column chromatography with >97% ^125m^Te recovered. Cd^125m^Te/ZnS-201B nanoparticles retained >97% of the radioactivity after 7 days in PBS at room temperature. Kennel et al. (5) reported that Cd^125m^Te/ZnS-201B nanoparticles had a diameter of 20–30 nm with a radiospecific activity of 78.5 MBq/nmol (2.1 mCi/nmol of antibody). There were ~3 nanoparticles per antibody molecule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cd+201B+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cd+201B+%20rodentia)]

Woodward et al. (4) studied long-term ex vivo biodistribution in normal mice (n = 5/group) at 1, 4, 24, 72, and 144 h after intravenous injection of 2.9 MBq (0.078 mCi) Cd^125m^Te/ZnS-201B nanoparticles/mouse. Lung (targeted organ) accumulation was 437 ± 26, 276 ± 37, 188 ± 24, 151 ± 18, and 136 ± 19% injected dose per gram tissue (% ID/g) at the respective time points. The spleen showed accumulation of 15 ± 2, 55 ± 8, 66 ± 9, 47 ± 8, and 39 ± 12% ID/g, while the liver accumulated 15 ± 1, 25 ± 2, 23 ± 3, 18 ± 2, and 19 ± 4% ID/g at these time points. Radioactivity accumulation in the kidney was lower than in the liver.

Ex vivo biodistribution studies of Cd^125m^Te/ZnS nanoparticles conjugated with control mAb 33 were also performed in mice at 4 h and 24 h. Lung accumulation of Cd^125m^Te/ZnS nanoparticles conjugated with control mAb 33 was ~100-fold lower than that of Cd^125m^Te/ZnS-201B nanoparticles alone, with 4 ± 1 and 2 ± 1% ID/g at 4 h and 24 h, respectively. However, the liver accumulation was 2–3 times higher than that of Cd^125m^Te/ZnS-201B nanoparticles. The blood concentration was <1% ID/g for both nanoparticles at 24 h after injection.

SPECT/computed tomography imaging scans were also performed with both nanoparticles in mice. The lung, spleen, and liver were clearly visualized with 201B nanoparticles, whereas only the liver and spleen were visualized with the control mAb nanoparticles. Kennel et al. (5) confirmed and extended those data. Ex vivo autoradiography studies in the lung showed that Cd^125m^Te/ZnS-201B nanoparticles accumulated more uniformly and in higher quantities in the lung than Cd^125m^Te/ZnS nanoparticles with control mAb. Depletion of phagocytic cells in the liver prior to injection of Cd^125m^Te/ZnS-201B nanoparticles enhanced the accumulation in the lung and decreased accumulation in the liver with little effect on the spleen accumulation. Immunohistostaining confirmed the depletion of phagocytic cells in the liver. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cd+201B+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cd+201B+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cd+201B+human)]

No publication is currently available.

## References

1 Singh N., Manshian B., Jenkins G.J., Griffiths S.M., Williams P.M., Maffeis T.G., Wright C.J., Doak S.H. (2009). NanoGenotoxicology: the DNA damaging potential of engineered nanomaterials. Biomaterials.
2 Koutsi A., Papapanagiotou A., Papavassiliou A.G. (2008). Thrombomodulin: from haemostasis to inflammation and tumourigenesis. Int J Biochem Cell Biol.
3 Hanly A.M., Winter D.C. (2007). The role of thrombomodulin in malignancy. Semin Thromb Hemost.
4 Woodward D., Kennel S.J., Mirzadeh S., Dai S. (2007). W. J.S., and R. T., In vivo SPECT/CT imaging and biodistribution using radioactive Cd125mTe/ZnD nanoparticles. Nanotechnology.
5 Kennel S.J., Woodward J.D., Rondinone A.J., Wall J., Huang Y., Mirzadeh S. (2008). The fate of MAb-targeted Cd(125m)Te/ZnS nanoparticles in vivo. Nucl Med Biol.